# 2-[^11^C]Methyl-5-[6-phenylpyridazine-3-yl]octahydropyrrolo[3,4-c]pyrrole

Chemical name: | 2-[^11^C]Methyl-5-[6-phenylpyridazine-3-yl]octahydropyrrolo[3,4-c]pyrrole
Abbreviated name: | [^11^C]A-582941
Synonym:
Agent category: | Compound
Target: | Neuronal α7 nicotinic acetylcholine receptor (nAChR)
Target category: | Receptor
Method of detection: | Positron emission tomography, PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=A-582941)]

Neuronal α4β2 nicotinic cholinergic receptors (nAChRs) are part of a heterogeneous family of ligand-gated ion channels expressed in the central nervous system, where their activation by acetylcholine and nicotine causes a rapid increase in cellular permeability to ions, such as Na^+^ and Ca^2+^ (1-3). Nicotinic receptors exist as pentamers (homomeric or heteromeric) in various brain regions and ganglia. There are nine subtypes of ligand-binding α receptors (α2 to α10) and four subtypes of structural β receptors (β2 to β5). nAChRs have been found to be involved in cognitive processes such as learning memory and control of movement in normal subjects. nAChR dysfunction has been implicated in a number of human diseases such as schizophrenia, Huntington's disease, Alzheimer's disease, and Parkinson's disease. nAChRs also play a significant role in nicotine addiction and other health problems associated with tobacco smoking.

3-[2(S)-2-Azetidinylmethoxy]pyridine (A-85380) is a highly potent and selective α4β2 nAChR agonist with subnanomolar affinity (4, 5). 6-[^18^F]Fluoro-A-85380 and 2-[^18^F]fluoro-A-85380 have been studied in humans as positron emission tomography (6) agents for α4β2 nAChR imaging in the brain for studying neuropsychiatric disorders. A-85380 has also been labeled as 5-[^123^I]iodo-A-85380, which was developed as a single-photon emission computed tomography agent for the non-invasive study of α4β2 nAChR in the brain. On the other hand, there are some implications that homomeric α7 nAChRs may also play a role in the pathophysiology of neuropsychiatric disorders (7-9). α7 nAChRs are highly expressed in the cerebral cortex, hippocampus, and subcortical limbic regions, which are involved in learning, memory, and information processing (10-12). 4-Bromophenyl-1,4-diazabicyclo(3.2.2)nonane-4-carboxylate (SSR180711) has been shown to be a potent and selective partial agonist for α7 nAChRs with nanomolar affinity (13). 4-[^11^C]Methylphenyl-1,4-diazabicyclo(3.2.2)nonane-4-carboxylate ([^11^C]CHIBA-1001) has been developed as a PET agent for the noninvasive study of α7 nAChR in the brain (14). In this chapter, another α7 nAChR agonist, 2-[^11^C]methyl-5-[6-phenylpyridazine-3-yl]octahydropyrrolo[3,4-c]pyrrole ([^11^C]A-582941) (15), is being evaluated as a useful PET imaging agent.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=nicotinic%20acetylcholine%20receptor+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (α7 nAChR (http://www.ncbi.nlm.nih.gov/gene/1139))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/118511)
- Clinical trials (α7 nAChR (http://www.clinicaltrials.gov/ct2/results?term=alpha+7+nicotinic+cholinergic+receptors))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=A-582941%20and%20synthesis)]

Toyohara et al. (15) reported the synthesis of [^11^C]A-582941 by methylation of desmethyl-A-582941 in the presence of NaOH with [^11^C]methyl triflate in an automated synthesis system. The mixture was allowed to react for 1 min at room temperature, and [^11^C]A-582941 was purified with high-performance liquid chromatography (HPLC). Average radiochemical yield was 16.8 ± 12.0% (n = 8). The radiochemical purity was >97% with a specific activity of 15–108 GBq/µmol (0.4–3.0 Ci/µmol) at the end of synthesis. Total synthesis time was ~30 min from the end of bombardment.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=A-582941%20and%20in%20vitro)]

Bitner et al. (16) reported that A-582941 exhibited K_i_ values of 10.8 and 16.7 nM for α7 nAChR (obtained with the use of [^3^H]A-585539) in rat and human brain membranes, respectively. A-582941 exhibited little affinity for α4, α3, and α2 nAChRs, and no affinity for other receptors.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=A-582941%20and%20rodentia)]

Toyohara et al. (15) performed ex vivo biodistribution of 2 MBq (0.054 mCi) [^11^C]A-582941 (0.05 nmol) in normal mice (n = 4/group) at 1–60 min. The highest uptake (percentage of injected dose per gram of tissue (% ID/g)) of [^11^C]A-582941 was found in the lungs (18.1), followed by the kidneys (13.9), liver (12.4), pancreas (7.5), spleen (5.5), small intestines (4.6), heart (4.3), brain (3.9), and muscle (2.0) at 1–15 min after injection. The radioactivity level of [^11^C]A-582941 in the blood was low (0.8) at 5 min after injection. HPLC analysis of the plasma showed that 40.5% and 26.8% of [^11^C]A-582941 was intact at 15 min and 30 min after injection with two major hydrophilic metabolites. On the other hand, little degradation of [^11^C]A-582941 was detected in the brain (>95% intact) at these time points. Blocking studies were performed with co-injection (1 mg/kg) of the selective α7 nAChR agonists (SSR180711, A-582941, A-844606) and the selective α4β2 nAChR agonist A-85380 at 15 min after injection. In the control mice, accumulation in the hippocampus, medulla oblongata, hypothalamus, striatum, midbrain, and cerebral cortex was not significantly higher than accumulation in the cerebellum indicating high level of non-specific binding of [^11^C]A-582941. SSR180711, A-582941, A-844606, and A-85380 did not significantly decrease the accumulation of [^11^C]A-582941 in the brain tissues, with the exceptions of SSR180711 in the medulla oblongata (P < 0.05) and A-582941 in the medulla oblongata and midbrain (P < 0.05). Neither of these results supported specific binding.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=A-582941%20and%20(dog%20or%20pig%20or%20sheep%20or%20rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=A-582941%20and%20(primate%20not%20human))]

[^11^C]A-582941 PET studies with rhesus monkeys (n = 4) showed substantial brain accumulation with selective uptake in the regions of the hippocampus, frontal cortex, thalamus, and cerebellum at 10–30 min after injection with gradual washouts (15). In Logan graphical analysis (total distribution volume (V_T_)), the cerebellum (23.0 ± 3.4 ml/g) showed lower binding than the hippocampus (28.0 ± 3.8 ml/g), frontal cortex (29.2 ± 4.7 ml/g), and thalamus (30.4 ± 4.1 ml/g). The regional distribution of [^11^C]A-582941 is consistent with the distribution of α7 nAChRs. [^11^C]A-582941 V_T_ values in the brain regions were reduced by 31%–36% with pretreatment with SSR180711 (5.0 mg/kg, 30 min). The fraction of unchanged [^11^C]A-582941 in the plasma as determined with thin-layer chromatography was ~90% at 30 min after injection. Detection of specific binding in the conscious monkeys (PET scans) and not in mice (ex vivo biodistribution) may be explained by the differences in species and blocking experiments (co-injection in mice versus pretreatment in monkeys).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=A-582941%20and%20human)]

No publication is currently available.

## References

1 Alkondon M., Albuquerque E.X. (2004). The nicotinic acetylcholine receptor subtypes and their function in the hippocampus and cerebral cortex. Prog Brain Res.
2 Gotti C., Riganti L., Vailati S., Clementi F. (2006). Brain neuronal nicotinic receptors as new targets for drug discovery. Curr Pharm Des.
3 Hogg R.C., Raggenbass M., Bertrand D. (2003). Nicotinic acetylcholine receptors: from structure to brain function. Rev Physiol Biochem Pharmacol.
4 Abreo M.A., Lin N.H., Garvey D.S., Gunn D.E., Hettinger A.M., Wasicak J.T., Pavlik P.A., Martin Y.C., Donnelly-roberts D.L., Anderson D.J., Sullivan J.P., Williams M., Arneric S.P., Holladay M.W. (1996). Novel 3-Pyridyl ethers with subnanomolar affinity for central neuronal nicotinic acetylcholine receptors. J Med Chem.
5 Sullivan J.P., Donnelly-Roberts D., Briggs C.A., Anderson D.J., Gopalakrishnan M., Piattoni-Kaplan M., Campbell J.E., McKenna D.G., Molinari E., Hettinger A.M., Garvey D.S., Wasicak J.T., Holladay M.W., Williams M., Arneric S.P. (1996). A-85380 [3-(2(S)-azetidinylmethoxy) pyridine]: in vitro pharmacological properties of a novel, high affinity alpha 4 beta 2 nicotinic acetylcholine receptor ligand. Neuropharmacology.
6 Akerman M.E., Pilch J., Peters D., Ruoslahti E. (2005). Angiostatic peptides use plasma fibronectin to home to angiogenic vasculature. Proc Natl Acad Sci U S A.
7 Gotti C., Zoli M., Clementi F. (2006). Brain nicotinic acetylcholine receptors: native subtypes and their relevance. Trends Pharmacol Sci.
8 Nomikos G.G., Schilstrom B., Hildebrand B.E., Panagis G., Grenhoff J., Svensson T.H. (2000). Role of alpha7 nicotinic receptors in nicotine dependence and implications for psychiatric illness. Behav Brain Res.
9 Nordberg A. (2001). Nicotinic receptor abnormalities of Alzheimer's disease: therapeutic implications. Biol Psychiatry.
10 Thomsen M.S., Hansen H.H., Timmerman D.B., Mikkelsen J.D. (2010). Cognitive improvement by activation of alpha7 nicotinic acetylcholine receptors: from animal models to human pathophysiology. Curr Pharm Des.
11 Barrantes F.J., Borroni V., Valles S. (2010). Neuronal nicotinic acetylcholine receptor-cholesterol crosstalk in Alzheimer's disease. FEBS Lett.
12 Hajos M., Rogers B.N. (2010). Targeting alpha7 nicotinic acetylcholine receptors in the treatment of schizophrenia. Curr Pharm Des.
13 Biton B., Bergis O.E., Galli F., Nedelec A., Lochead A.W., Jegham S., Godet D., Lanneau C., Santamaria R., Chesney F., Leonardon J., Granger P., Debono M.W., Bohme G.A., Sgard F., Besnard F., Graham D., Coste A., Oblin A., Curet O., Vige X., Voltz C., Rouquier L., Souilhac J., Santucci V., Gueudet C., Francon D., Steinberg R., Griebel G., Oury-Donat F., George P., Avenet P., Scatton B. (2007). SSR180711, a novel selective alpha7 nicotinic receptor partial agonist: (1) binding and functional profile. Neuropsychopharmacology.
14 Hashimoto K., Nishiyama S., Ohba H., Matsuo M., Kobashi T., Takahagi M., Iyo M., Kitashoji T., Tsukada H. (2008). [11C]CHIBA-1001 as a novel PET ligand for alpha7 nicotinic receptors in the brain: a PET study in conscious monkeys. PLoS ONE.
15 Toyohara J., Ishiwata K., Sakata M., Wu J., Nishiyama S., Tsukada H., Hashimoto K. (2010). In vivo evaluation of alpha7 nicotinic acetylcholine receptor agonists [11C]A-582941 and [11C]A-844606 in mice and conscious monkeys. PLoS ONE.
16 Bitner R.S., Bunnelle W.H., Anderson D.J., Briggs C.A., Buccafusco J., Curzon P., Decker M.W., Frost J.M., Gronlien J.H., Gubbins E., Li J., Malysz J., Markosyan S., Marsh K., Meyer M.D., Nikkel A.L., Radek R.J., Robb H.M., Timmermann D., Sullivan J.P., Gopalakrishnan M. (2007). Broad-spectrum efficacy across cognitive domains by alpha7 nicotinic acetylcholine receptor agonism correlates with activation of ERK1/2 and CREB phosphorylation pathways. J Neurosci.